# Indocyanine green–doped calcium phosphate nanoparticles

Chemical name: | Indocyanine green–doped calcium phosphate nanoparticles
Abbreviated name: | ICG-CPNPs
Synonym:
Agent category: | Compound
Target: | Enhanced retention and permeability (EPR)
Target category: | Non-targeted
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Indocyanine green (ICG)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

Among the various NIR agents, indocyanine green (ICG), with absorption at 780 nm and emission at 820 nm, is the only agent approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (4). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications. However, ICG has a plasma half-life of 2–4 min because it aggregates in the blood and is rapidly cleared from blood circulation (5). ICG is prone to photobleaching and nonspecific quenching via its extensive binding to proteins. Calcium phosphate (CP) is present at millimolar concentrations in the blood. CP nanoparticles (CPNPs) have been used to encapsulate organic molecules for intracellular imaging and drug delivery (6). Altinoglu et al. (7) used CPNPs doped with ICG to improve the bioavailability of ICG as a NIR imaging agent in small animals.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=ICG+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Clinical trials (Indocyanine green (http://www.clinicaltrials.gov/ct2/results?term=indocyanine+green))
- Drug information in FDA (http://google2.fda.gov/search?q=indocyanine+green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=13)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs+synthesis)]

Two reverse microemulsions were formed by a cyclohexane/nonylphenoxyl (glycolether) (Igepal CO-520)/water system CaCl_2_ (0.065 mM) was added to 14 mL of a 29 vol % solution of Igepal CO-520 in cyclohexane to form microemulsion A (7). Microemulsion B was produced by adding disodium phosphate (0.39 mM) and disodium silicate (0.54 mM) to an identical Igepal CO-520/cyclohexane mixture. ICG (5.2 mM) was added to microemulsion B. The microemulsions were equilibrated under constant stirring for 1 h before being combined to form a microemulsion mixture (microemulsion C). Microemulsion C was stirred for 2 min before the dispersant, 0.225 mM sodium citrate, was added, and the solution was stirred for an additional 15 min. The product, ICG-CPNPs, was isolated with column chromatography. The size of ICG-CPNPs was 16 ± 0.23 nm as measured with transmission electron microscopy.

To prepare polyethylene glycol–conjugated ICG-CPNPs (PEG-ICG-CPNPs), a 4-mL aliquot of the carboxylateCPNPs (5 × 10^13^ particles) was chemically conjugated with methoxypolyethylene glycol amine (mPEG-amine) through an ethyl-N-(3-dimethylaminopropyl)-N'-hydrochloride carbodiimide (EDAC) reaction. EDAC (1 mg) and mPEG-amine (10 mg) were added to the sample under continuous stirring (six-fold excess for monolayer surface coverage). The particles were reacted for 15 h at 50°C to form amide linkages between the carboxylate surfaces and the mPEG-amine. The mixture was then filtered through a centrifuge filter to remove excess EDAC and unreacted mPEG-amine.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs+in+vitro)]

TEM images showed that the doped ICG was uniformly distributed in the CP matrix of each NP (7). The concentration of ICG was estimated by fluorescence emission intensity to be 0.01 mM in 10^13^ NPs/mL. The fluorescence emission intensity of each ICG-CPNP was 1,000 times that of one ICG molecule because it contains more than 1 ICG. The quantum efficiency of ICG-CPNPs (0.049 ± 0.003) was one-fold greater than that of free ICG (0.028 ± 0.001) in saline buffer. The emission spectra and photostability for ICG-CPNPs were more stable than those of free ICG in various media. Ex situ imaging studies were performed with porcine muscle tissue. ICG and ICG-CPNPs solutions (0.1 mM) were injected at different depths in the porcine muscle tissue. Detectable fluorescence signal was still observed at 3 cm for ICG-CPNPs as compared with 1.5 cm for free ICG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs+rodentia)]

Altinoglu et al. (7) performed in vivo whole-body NIR fluorescence imaging studies of PEG-ICG-CPNPs and ICG (200 nmol/mouse) in nude mice (n = 4/group) bearing human MDA-MB-231 breast adenocarcinoma tumors. Images were obtained at 3, 24, and 96 h after intravenous injection. PEG-ICG-CPNPs exhibited clear signal intensity at 24 h after injection. The tumors were still clearly visualized at 96 h. High fluorescence intensities were observed ex vivo in the liver and kidneys at 10 min after injection. On the other hand, no detectable signal was observed in the tumors with ICG at 24 h and 96 h. The authors suggested that PEG-ICG-CPNPs provide prolonged circulation times with passive tumor accumulation at 24 h and 96 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-CPNPs+human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Sakka S.G. (2007). Indocyanine green plasma disappearance rate as an indicator of hepato-splanchnic ischemia during abdominal compartment syndrome. Anesth Analg.
5 Desmettre T., Devoisselle J.M., Mordon S. (2000). Fluorescence properties and metabolic features of indocyanine green (ICG) as related to angiography. Surv Ophthalmol.
6 Morgan T.T., Muddana H.S., Altinoglu E.I., Rouse S.M., Tabakovic A., Tabouillot T., Russin T.J., Shanmugavelandy S.S., Butler P.J., Eklund P.C., Yun J.K., Kester M., Adair J.H. (2008). Encapsulation of organic molecules in calcium phosphate nanocomposite particles for intracellular imaging and drug delivery. Nano Lett.
7 Altinoglu E.I., Russin T.J., Kaiser J.M., Barth B.M., Eklund P.C., Kester M., Adair J.H. (2008). Near-infrared emitting fluorophore-doped calcium phosphate nanoparticles for in vivo imaging of human breast cancer. ACS Nano.